# [7-methyl-^11^C]-(E)-8-(3,4,5-Trimethoxystyryl)-1,3,7-trimethylxanthine

Chemical name: | [7-methyl-^11^C]-(E)-8-(3,4,5-Trimethoxystyryl)-1,3,7-trimethylxanthine
Abbreviated name: | [^11^C]TMSX
Synonym: | [^11^C]KF18446
Agent category: | Compound
Target: | Adenosine A_2A_ receptor
Target category: | Receptor
Method of detection: | PET
Source of signal: | ^11^C
Activation: | No
Studies: | - In vitro; - Rodents; - Non-human primates; - Humans | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22KF18446%22%5BSubstance%20Name%5D%20OR%2011C-TMSX%5BText%20Word%5D)]

Adenosine is an endogenous nucleoside that modulates a number of physiologic functions in the central nervous system (CNS) and in peripheral organs such as the heart, kidney, and muscle (1, 2). The effect is mediated by two major subtypes of receptors (A_1_ and A_2A_ receptors) and two minor subtypes (A_2B_ and A_3_). In the CNS, A_1_ receptors are present both pre- and postsynaptically in the hippocampus, cerebral cortex, thalamus, striatum, and cerebellum. A_2A_ receptors are highly concentrated and co-localized with dopamine D_1_ and D_2_ receptors in the striatum, nucleus accumbens, and olfactory tubercle. A_2A_ receptors are also present in low amounts in the hippocampus and cortex. A_2B_ receptors are widely distributed, but the density is higher in the gastrointestinal tract. A_3_ receptors are also widely distributed but with higher density in the testis. A_1_ and A_3_ receptors mediate inhibition of adenylyl cyclase, whereas A_2A_ and A_2B_ receptors mediate stimulation. Changes in the adenosine receptor functions are implicated in epilepsy, ischemic cerebral stroke, movement disorders, sleep disorders, and psychiatric disorders (3-5).

A_2A_ receptors have been studied in vivo by positron emission tomography (PET) using [7-methyl-^11^C]-(E)-8-(3,4,5-trimethoxystyryl)-1,3,7-trimethylxanthine ([^11^C]TMSX), a methylxanthine analog of KF17387 with selective A_2A_ antagonistic activity (6). TMSX showed better selectivity for A_2A_ over A_1_ receptors than KF17387 and had little affinity in various neuroreceptor-binding assays (7). [^11^C]TMSX is being developed as a PET agent for the non-invasive study of A_2A_ receptors in the human brain and heart.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C-TMSX%20and%20synthesis)]

In the report by Ishiwata et al. (8), [^11^C]TMSX was synthesized by alkylation of the 7-desmethyl precursor ((E)-8-(3,4,5-trimethoxystyryl)-1,3-dimethylxanthine) with [^11^C]methyl iodide. Purification by high-performance liquid chromatography (HPLC) provided a decay-corrected radiochemical yield of 25-46%, radiochemical purity >99%, and specific activity of 10-72 GBq/μmol (0.27-1.95 Ci/μmol) in 20-25 min.

Kawamura et al. (9) described the synthesis of [^11^C]TMSX from the desmethyl precursor with [^11^C]methyl triflate in the presence of Cs_2_CO_3_. This procedure provided improved radiochemical yield (decay-corrected) of 55.3 ± 5.2% based on [^11^C]methyl triflate. No time of synthesis or specific activity was reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C-TMSX%20and%20in%20vitro)]

In the study by Ishiwata et al. (8), the K_i_ values of TMSX and KF17837 were 5.9 and 1.0 nM, respectively, for the A_2A_ receptors and 1,600 and 62 nM for the A_1_ receptors. Hence, TMSX showed better selectivity for A_2A_ over A_1_ receptors than KF17387. In vitro autoradiography (ARG) studies of brain sections with [^11^C]TMSX showed high binding in the caudate putamen, nucleus accumbens, and olfactory tubercle with a striatum/cortex ratio of 8.4 ± 2.2. TMSX (20 μM) blocked 91% of [^11^C]TMSX binding in the striatum but only 54% in the cortex. Saturation binding experiments of [^11^C]TMSX in the rat striatum and cortex gave estimated K_d_ values of 9.8 and 16.4 nM, with B_max_ values of 170 and 33 fmol/mm^3^ tissue, respectively (7).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C-TMSX%20and%20rodentia)]

Biodistribution studies in normal mice showed high initial accumulation of radioactivity in the liver, followed by the kidney (12.08% injected dose (ID)/g), heart (10.94% ID/g), liver (4.42% ID/g), pancreas (4.23%ID/g), and lung (3.92% ID/g) at 1 min after injection of [^11^C]TMSX (10). The levels of radioactivity were low in the brain (2.49% ID/g) and blood (1.58% ID/g). Radioactivity levels decreased gradually in all studied organs, with the exception of the liver, which showed an increase for the first 15 min followed by a gradual decrease. Ex vivo ARG indicated that uptake of [^11^C]TMSX was higher in the striatum than the cortex and cerebellum with a striatum/cortex ratio of 3.16 ±0.24 (8). This high, selective binding of [^11^C]TMSX in the striatum was also confirmed by in vitro ARG and iv vivo regional brain distribution studies. Coadiministration of the A_2A_ antagonist KF17837, but not the A_1_ antagonist KF15372, decreased the accumulation in the brain in a dose-dependent manner at 15 min post injection. Pretreatment with 10 and 100 mg/kg theophylline (a low-affinity adenosine antagonist) 15 min before [^11^C]TMSX injection in mice significantly reduced striatal accumulation. About 80% and >98% of radioactivity in the plasma and striatum, respectively, was intact [^11^C]TMSX at 30 min post injection.

Ishiwata et al. (11) reported ex vivo ARG studies in the rat globus pallidus. The highest uptake by the globus pallidus was for [^11^C]SCH 23390 (dopamine D_1_ receptor) followed by [^18^F]fluorodeoxyglucose (FDG), [^11^C]TMSX, and [^11^C]raclopride (dopamine D_2_ receptor). Receptor-specific uptake by the globus pallidus was observed for [^11^C]TMSX and [^11^C]SCH 23390, but not for [^11^C]raclopride. The globus pallidus/striatum uptake ratios for FDG and [^11^C]TMSX were ~0.6, which was twice as large as that for [^11^C]SCH 23390. In a rat model of degeneration of gamma-aminobutyric acid-ergic-enkephalin neurons induced by intrastriatal injection of quinolinic acid, the accumulation and binding potentials of [^11^C]TMSX and [^11^C]raclopride in the lesioned striatum were remarkably reduced but were higher than the values for [^11^C]SCH 23390 (11, 12).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C-TMSX%20and%20%28dog%20or%20or%20rabbit%20or%20sheep%20or%20pig%29)]

No publications are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C-TMSX%20and%20%28primate%20not%20human%29)]

Using PET, Ishiwata et al. (8) obtained serial brain scans in 1 monkey after injection of 102 MBq (2.8 mCi) of [^11^C]TMSX. The accumulation of radioactivity in the striatum peaked at 5-10 min and then decreased for the final 60 min of study. The uptake was the highest in the striatum, followed by the thalamus, cerebellum, and cortex. The striatum/cortex and striatum/cerebellum ratios gradually increased from 1.3 and 1.2, respectively, at 5 min to 1.56 and 1.46 at 60 min.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C-TMSX%20and%20human)]

Ishiwata et al. (13) reported on PET myocardial imaging in 1 healthy volunteer after injection of 590 MBq (16 mCi) of [^11^C]TMSX. The levels in the left ventricular wall, left ventricular anterior wall, and interventricular septum increased during the first 3 min after injection and then decreased gradually. In contrast, the radioactivity in the lung decreased rapidly. The fraction of unchanged [^11^C]TMSX in blood samples, as determined by HPLC, was 97, 94, and 95% at 10, 30, and 60 min, respectively. In other studies of 2 subjects, infusion of theophylline (3.3 mg/kg) reduced the distribution volumes (DVs; baseline values, 3.62-3.73) of the three heart regions by 18-22% as determined by Logan analysis (14). The DV (1.57) of the brachii muscle was reduced by 10%. The A_2A_ receptors have also been preliminarily visualized in human brain with relatively high DVs in the caudate (1.72) and putamen (1.72), followed by the thalamus (1.64), cerebellum (1.52), brainstem (1.42), and cerebral cortex (1.26) (15). Mishina et al. (16) was used a two-tissue, three-compartment model to estimate the distribution of A_2A_ receptors in the brain (n = 5) using metabolite-correction arterial input function. The binding potential (BP) was the largest in the anterior (1.25) and posterior putamen (1.20), followed by la the head of caudate nucleus (1.05), thalamus (1.03), and frontal cortex lobe (0.46). On the other hand, Naganawa et al. (17) showed that Logan plot estimated BPs matching those derived from compartment analysis (n = 5) with or without arterial blood sampling. Without the metabolite correction, the estimate of BP underestimated the true value by only 5%. Internal dosimetry data for [^11^C]TMSX in humans are not available in the literature.

## References

1 Fredholm B.B., Abbracchio M.P., Burnstock G., Daly J.W., Harden T.K., Jacobson K.A., Leff P., Williams M. (1994). Nomenclature and classification of purinoceptors. Pharmacol Rev.
2 Palmer T.M., Stiles G.L. (1995). Adenosine receptors. Neuropharmacology.
3 Dunwiddie T.V., Masino S.A. (2001). The role and regulation of adenosine in the central nervous system. Annu Rev Neurosci.
4 El Yacoubi M., Costentin J., Vaugeois J.M. (2003). Adenosine A2A receptors and depression. Neurology.
5 von Lubitz D.K. (2001). Adenosine in the treatment of stroke: yes, maybe, or absolutely not?. Expert Opin Investig Drugs.
6 Noguchi J., Ishiwata K., Wakabayashi S., Nariai T., Shumiya S., Ishii S., Toyama H., Endo K., Suzuki F., Senda M. (1998). Evaluation of carbon-11-labeled KF17837: a potential CNS adenosine A2a receptor ligand. J Nucl Med.
7 Ishiwata K., Ogi N., Shimada J., Nonaka H., Tanaka A., Suzuki F., Senda M. (2000). Further characterization of a CNS adenosine A2a receptor ligand [11C]KF18446 with in vitro autoradiography and in vivo tissue uptake. Ann Nucl Med.
8 Ishiwata K., Noguchi J., Wakabayashi S., Shimada J., Ogi N., Nariai T., Tanaka A., Endo K., Suzuki F., Senda M. (2000). 11C-labeled KF18446: a potential central nervous system adenosine A2a receptor ligand. J Nucl Med.
9 Kawamura K., Ishiwata K. (2004). Improved synthesis of [11C]SA4503, [11C]MPDX and [11C]TMSX by use of [11C]methyl triflate. Ann Nucl Med.
10 Ishiwata K., Wang W.F., Kimura Y., Kawamura K., Ishii K. (2003). Preclinical studies on [11C]TMSX for mapping adenosine A2A receptors by positron emission tomography. Ann Nucl Med.
11 Ishiwata K., Ogi N., Shimada J., Wang W., Ishii K., Tanaka A., Suzuki F., Senda M. (2000). Search for PET probes for imaging the globus pallidus studied with rat brain ex vivo autoradiography. Ann Nucl Med.
12 Ishiwata K., Ogi N., Hayakawa N., Oda K., Nagaoka T., Toyama H., Suzuki F., Endo K., Tanaka A., Senda M. (2002). Adenosine A2A receptor imaging with [11C]KF18446 PET in the rat brain after quinolinic acid lesion: comparison with the dopamine receptor imaging. Ann Nucl Med.
13 Ishiwata K., Kawamura K., Kimura Y., Oda K., Ishii K. (2003). Potential of an adenosine A2A receptor antagonist [11C]TMSX for myocardial imaging by positron emission tomography: a first human study. Ann Nucl Med.
14 Ishiwata K., Mizuno M., Kimura Y., Kawamura K., Oda K., Sasaki T., Nakamura Y., Muraoka I., Ishii K. (2004). Potential of [11C]TMSX for the evaluation of adenosine A2A receptors in the skeletal muscle by positron emission tomography. Nucl Med Biol.
15 Ishiwata K., Mishina M., Kimura Y., Oda K., Sasaki T., Ishii K. (2005). First visualization of adenosine A(2A) receptors in the human brain by positron emission tomography with [11C]TMSX. Synapse.
16 Mishina M., Ishiwata K., Kimura Y., Naganawa M., Oda K., Kobayashi S., Katayama Y., Ishii K. (2007). Evaluation of distribution of adenosine A2A receptors in normal human brain measured with [11C]TMSX PET. Synapse.
17 Naganawa M., Kimura Y., Mishina M., Manabe Y., Chihara K., Oda K., Ishii K., Ishiwata K. (2007). Quantification of adenosine A2A receptors in the human brain using [11C]TMSX and positron emission tomography. Eur J Nucl Med Mol Imaging.